# L-[methyl-^11^C]Methionine

Chemical name: | L-[methyl-^11^C]Methionine
Abbreviated name: | [^11^C]MET
Synonym: | 2-Amino-4-[^11^C]methylsulfanyl-butanoic acid, l-[S-methyl^11^C]methionine
Agent category: | Amino acid
Target: | L-type amino acid transporter system and Na^+^-dependent system B^0^
Target category: | Neutral amino acid uptake and protein synthesis
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine)]

A variety of [^11^C] and [^18^F] labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids such as, L-[^11^C]leucine, L-[^11^C]methionine (MET), and L-[^11^C]tyrosine and non-natural amino acids such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (1, 4, 5).

Some 20 amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and a sodium-dependent transporter system A but also a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their higher metabolic activities including incorporation into proteins than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis and cell division. Tumor cells were found to have over-expressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in detection of tumors (2, 6) but are not approved by the United States Food and Drug Administration. They are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell. These natural amino acid images are based on amino acid transport and protein incorporation.

[^11^C]MET has been widely used in detection of brain, head and neck, lung, and breast cancer as well as lymphomas [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human%20and%20neoplasm)]. It can cross the blood-brain barrier. It is incorporated mainly into proteins but also into lipid, RNA, and DNA. [^11^C]MET PET imaging is more sensitive to radiotherapy compared to FDG and is useful for monitoring treatment of cancer.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), L-[^11^C]methionine (http://google2.fda.gov/search?q=11C-methionine+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20synthesis)]

A continuous flow procedure was automated for the synthesis of [^11^C]methyl iodide from [^11^C]CO_2_ and L-[methyl-^11^C]methionine from [^11^C]methyl iodide and L-S-benzyl-homocysteine (8). The preparation was completed in 20 min after the end of bombardment with a yield of >30%. This procedure produced about 44 mCi or 1.62 MBq [^11^C]MET with a specific activity of 3.3 Ci/mmol (122 GBq/mmol). Radiochemical purity is >96%.

A simple synthesis was performed without high-performance liquid chromatography (HPLC) purification (9), using a solid supported ^11^C-methylation of L-homocysteine thiolactone on Al_2_O_3_. The preparation required only filtration for separation of L-homocysteine and [^11^C]MET. Average absolute yields from 258 syntheses were 10.2 GBq (276 mCi), starting from 47.6 GBq (1.29 Ci) of [^11^C]CO_2_ at the end of bombardment, representing 21.2 ± 7.9%, not corrected for decay. The radiochemical purity was >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20in%20vitro)]

There was a time dependent increase of uptake (0.73% at 0.5 h and 11% at 4 h) of [^3^H]MET into HTB-14 human astrocytoma cells (10). [^3^H]MET was incorporated into proteins (44%), lipid (2.6%), RNA (5.8%), and DNA (11%) at 4 h. About 35% of the radioactivity remained in free intracellular pool at 4 h.

[^11^C]MET was found to be transported into F98 rat gliomas by the sodium independent transport system L (70%) and the Na^+^-dependent system B^0^ (30%) (6). About 15% of MET was incorporated into proteins at 2 h after incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20rodentia)]

Tissue accumulation of [^11^C]MET was studied in nude mice with MCF-7 human breast carcinoma tumors at 1 h after injection of 0.37 MBq (0.01 mCi) of the tracer (11). The organ with the highest uptake was in the liver (8.02% injected dose (ID)/g), followed by the kidneys (7.60% ID/g), spleen (7.36% ID/g), and stomach (6.75% ID/g). The tumor, muscle, and blood uptakes were 2.60, 1.56, and 2.73% ID/g, respectively.

AH109A rat hepatoma tumor cells were inoculated subcutaneously into rats to study the effect of radiotherapy on protein synthesis (12). [^11^C]MET was injected intravenously through the tail vein. The organ with the highest uptake was in the pancreas (7.5% ID/g), followed by the liver (4.5% ID/g). The tumor had an uptake of 2.7% ID/g and was clearly distinguished from other tissues. After 20 Gy (2,000 rads) of single-dose irradiation to the rat tumor, [^11^C]MET uptake fell to 54 ± 19% of non-irradiated tumor uptake at 12 h after irradiation. Necrosis accounted for 49 ± 7% of total tissue volume after 3 days. Tumor volume decreased 48 ± 12% 10 days after irradiation. [^11^C]MET uptake by tumor showed a sharp and rapid linear decrease after irradiation, and the response of the uptake to irradiation preceded the extension of necrosis and tumor shrinkage.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

Muscle protein synthesis rates (PSRs) were measured by [^11^C]MET PET in the paraspinal and hindlimb muscles of dogs (13). The PSRs were similar for paraspinal and hindlimb muscles, 0.172 and 0.208 nmol/min/g, respectively. The PSR determined by [^3^H]MET measurements was 0.27 nmol/min/g, indicating <10% transmethylation of MET. In a later study in rats, the PSR was 0.22 nmol/min/g in normal rats and 0.0032 nmol/min/g in cycloheximide-treated rats, supporting the hypothesis that MET accumulates in skeletal muscle as ^11^C-labeled proteins (14).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20AND%20%28primate%20not%20human%29)]

[^11^C]-L- or [^11^C]-D-methionine was injected intravenously into pregnant Rhesus monkeys (15). There was an instantaneous high uptake of radioactivity in the maternal aorta, and placenta. Both [^11^C]-L- and D-methionine rapidly crossed the placenta and accumulated in the fetal liver. The fetal liver uptake of [^11^C]-L-MET was higher than the [^11^C]-D-MET. In the [^11^C]-L-MET experiments, about 70% of the radioactivity in plasma was found in the high molecular fraction one hour after injection. A greater part of [^11^C]-D-compared to [^11^C]-L-activity was excreted in the urine. These data suggested that a major part of [^11^C]-D-MET was not used in fetal liver for protein synthesis.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human)]

Seventeen patients with suspected astrocytomas (9 of grade II and 8 of grade III) were studied by PET with [^18^F]FDG and [^11^C]MET (10). In all patients, PET images of [^11^C]MET and [^18^F]FDG provided higher tumor/white matter ratios than tumor/corresponding contralateral region ratios and tumor/mean cortical uptake ratios. In grade II patients, [^18^F]FDG did not exhibit a significant increase in tumor uptake, whereas [^11^C]MET was a good tumor predictor with ratios of about 1.50 ± 0.48. In grade III patients, both [^18^F]FDG and [^11^C]MET exhibited higher uptake ratios than for grade II, with [^11^C]MET(ratios of 2.50 ± 0.85) being better than [^18^F]FDG, possibly suggesting enhanced protein synthesis.

[^11^C]MET PET studies were performed the first 8 to 24 h after the onset of neurological symptoms and at the follow-up study 14 days after the ischemic attack (16). Increased [^11^C]MET uptake was found significantly in patchy areas in the immediate vicinity of infarction as well as in distant areas within the same hemisphere. In those areas, regional cerebral blood flow and oxygen extraction fraction were highly variable, and the regional cerebral metabolic rate of oxygen was preserved or slightly reduced. It was postulated that there were alterations of amino acid transport or protein synthesis in the brain tissue because of either blood-brain barrier disruption or post-ischemic hyper-perfusion.

Human dosimetry of [^11^C]MET was estimated in five normal volunteers (17). The average injected dose was 558 MBq (15.08 mCi). The organs that received the highest absorbed doses were found to be the bladder wall (0.027 mGy/MBq or 100 mrad/mCi), the pancreas (0.019 mGy/MBq or 70 mrad/mCi), the liver (0.018 mGy/MBq or 66 mrad/mCi), and the kidneys (0.011 mGy/MBq or 41 mrad/mCi). The effective dose was calculated as 0.0053 mSv/MBq (20 mrem/mCi) for a 70-kg-standard man.

For many years, [^11^C]MET was used for brain imaging of gliomas, astrocytomas, oligodendrogliomas, and other malignant brain tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human%20brain%20tumor)]. [^11^C]MET PET is useful to evaluate low-grade brain tumors and their responses to treatment (18). However, about 20% of low-grade brain tumors were not detectable, and some infarcts, hematomas, and inflammatory tissues may show high uptake (3). [^11^C]MET is proved to be a reliable and highly accurate imaging PET tracer for localizing parathyroid adenomas in patients in whom conventional imaging techniques have failed (19).

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Davis J., Yano Y., Cahoon J., Budinger T.F. (1982). Preparation of 11C-methyl iodide and L-[S-methyl-11C]methionine by an automated continuous flow process. Int J Appl Radiat Isot.
9 Mitterhauser M., Wadsak W., Krcal A., Schmaljohann J., Eidherr H., Schmid A., Viernstein H., Dudczak R., Kletter K. (2005). New aspects on the preparation of [11C]Methionine--a simple and fast online approach without preparative HPLC. Appl Radiat Isot.
10 Narayanan T.K., Said S., Mukherjee J., Christian B., Satter M., Dunigan K., Shi B., Jacobs M., Bernstein T., Padma M., Mantil J. (2002). A comparative study on the uptake and incorporation of radiolabeled methionine, choline and fluorodeoxyglucose in human astrocytoma. Mol Imaging Biol.
11 Amano S., Inoue T., Tomiyoshi K., Ando T., Endo K. (1998). In vivo comparison of PET and SPECT radiopharmaceuticals in detecting breast cancer. J Nucl Med.
12 Kubota K., Yamada K., Fukada H., Endo S., Ito M., Abe Y., Yamaguchi T., Fujiwara T., Sato T., Ito K., et al. (1984). Tumor detection with carbon-11-labelled amino acids. Eur J Nucl Med.
13 Hsu H., Yu Y.M., Babich J.W., Burke J.F., Livni E., Tompkins R.G., Young V.R., Alpert N.M., Fischman A.J. (1996). Measurement of muscle protein synthesis by positron emission tomography with L-[methyl-11C]methionine. Proc Natl Acad Sci U S A.
14 Carter E.A., Yu Y.M., Alpert N.M., Bonab A.A., Tompkins R.G., Fischman A.J. (1999). Measurement of muscle protein synthesis by positron emission tomography with L-[methyl-11C]methionine: effects of transamination and transmethylation. J Trauma.
15 Berglund L., Halldin C., Lilja A., Lindberg B.S., Lundqvist H., Langstrom B., Malmborg P., Nagren K., Stalnacke C.G. (1984). 11C-methionine kinetics in pregnant rhesus monkeys studied by positron emission tomography: a new approach to feto-maternal metabolism. Acta Obstet Gynecol Scand.
16 Jacobs A. (1995). Amino acid uptake in ischemically compromised brain tissue. Stroke.
17 Deloar H.M., Fujiwara T., Nakamura T., Itoh M., Imai D., Miyake M., Watanuki S. (1998). Estimation of internal absorbed dose of L-[methyl-11C]methionine using whole-body positron emission tomography. Eur J Nucl Med.
18 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
19 Beggs A.D., Hain S.F. (2005). Localization of parathyroid adenomas using 11C-methionine positron emission tomography. Nucl Med Commun.